# Pegylated bis(4-(N-(2-naphthyl)phenylamino)phenyl)-fumaronitrile (NPAPF) nanoparticles

Chemical name: | Pegylated bis(4-(N-(2-naphthyl)phenylamino)phenyl)-fumaronitrile (NPAPF) nanoparticles
Abbreviated name: | NPAPF-PEG NPs
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Optical imaging; near-infrared fluorescence imaging
Source of signal / contrast: | bis(4-(N-(2-naphthyl)phenylamino)phenyl)-fumaronitrile (NPAPF)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=folate%20receptor&cmd=DetailsSearch)]

Free organic near-infrared fluorescent (NIRF) dyes such as indocyanine green are usually used as nontargeted molecular imaging probes (e.g., for lymph node mapping or angiography). However, these compounds are highly hydrophobic, have low stability under in vivo conditions, and are not considered suitable for the detection of cancerous tumors due to their low quantum yields (QY) after excitation (1). To circumvent these problems, the organic NIRF dyes are often covalently linked to or enclosed in nanoparticles (NPs; nanocarriers or nanoprobes) for delivery into the circulatory system, but the fluorescence signals generated from these preparations are quenched even when high concentrations of the dyes are enclosed in the nanocarriers because these the chemicals tend to aggregate (2). Therefore, the amount of NIRF dye that can be loaded into NPs is rather limited. An ideal NIRF dye should have a characteristic high brightness, show little or no aggregation at high concentrations, and have a high QY, and the signal generated from the compound should be easily detected even when it is encapsulated in the NPs (2). Conversely, some NIRF dyes exhibit very low or no fluorescence while in solution, but on aggregation emit a strong fluorescence signal (the phenomenon is called “aggregation-induced emission” (AIE) and has been explained in detail by Hong et al. (3)). Although AIE dyes have been shown to be suitable for the detection of proteins, DNA, etc., or for the staining of living cells, they have not been evaluated for the in vivo imaging of organs or tissues in animals or humans (3).

NPs may be made of either inorganic materials (e.g., quantum dots; silica or gold or iron oxide) or organic materials (e.g., polymer core NPs, polymer or lipid micelles, liposomes, etc.) as described in detail by Merian et al. (4). Organic NPs have often been loaded with NIFR dyes, conjugated with a targeting molecule (such as an antibody, receptor ligand, or a molecule that has an affinity for a specific component, usually on the cell membrane), and used to detect or monitor the treatment of neoplastic tumors, or to noninvasively visualize one or more organs or areas of interest in animals or humans (4). On the basis of the above information, Yang et al. used bis(4-(N-(2-naphthyl)phenylamino)phenyl)-fumaronitrile (NPAPF), a NIRF dye with AIE properties, to prepare NPs (NPAPF NPs), and then the investigators functionalized the nanoprobes with polyethylene glycol (NPAPF-PEG NPs) (2). To investigate the in vitro targeting properties of the NPs, they were conjugated to folic acid (NPAPF-PEG-FA NPs), and the targeted nanoprobes were used to visualize human epithelial cells (KB cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology)) under fluorescence microscopy. The biodistribution and imaging characteristics of the NPAPF-PEG NPs were studied in mice bearing human lung carcinoma cell line tumors (A549 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-185&Template=cellBiology)).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=folate+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human folate receptor protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/X69516.1) sequences

Folate receptor–related clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor)

Folate receptors 1 (http://omim.org/entry/136430), 2 (http://omim.org/entry/136425) and 3 (http://omim.org/entry/602469) in Online Mendelian Inheritance in Man database (OMIM)

Human folate receptor 2 in Gene (http://www.ncbi.nlm.nih.gov/gene/2350) database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20synthesis&cmd=DetailsSearch)]

The synthesis and pegylation of NPAPF NPs (to obtain the NPAPF-PEG NPs) have been described by Yang et al. (2). Conjugation of the NPs with FA is detailed elsewhere (2). The number of PEG or FA molecules attached to each NPAPF NP or NPAPF-PEG NP, respectively, was not reported. The NPAPF NPs were reported to have a nearly spherical shape, with a size distribution range of 60–100 nm as determined with scanning electron microscopy (2). The emission peak of the NPs was at a wavelength of 650 nm, and the QY of the nanoprobes in water was determined to be up to 14.9%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20in%20vitro%20studies&cmd=DetailsSearch)]

The effects of phosphate-buffered saline (PBS; pH not mentioned), serum (source not reported), and pH ranging from 4 to 10 on the NPAPF NPs and NPAPF-PEG NPs were investigated by Yang et al. (2). The PBS, serum, or solutions with the different pH values did not affect the size of the NPAPF-PEG NPs for up to at least 48 h. However, during the same period, the NPAPF NPs showed a continuous increase in size when exposed to solutions with increasing pH values. The investigators attributed this phenomenon to the destruction of the surface charge on the NPs by the zwitterions in the solutions.

Exposure of KB cells to NPAPF NPs at concentrations ranging from 2.5 μM to 20 μM showed that >85% of the cells remained viable even after 48 h as determined with an MTT (3-(4, 5-dimethylthiazolyl-2)-2,5-diphenyltetrazolium bromide) cell proliferation assay, indicating that the NPs were nontoxic to the cells (2).

In another study, NPAPF-PEG NPs were shown to have superior photostability compared with the fluorescein isothiocyanate, a NIRF dye that is commonly used for bioimaging (2).

The NPAPF-PEG NPs and NPAPF-PEG-FA NPs were evaluated for the in vitro targeting of KB cells exhibiting a high expression of the folate receptor (FR; generated by growing the cells in FA-free growth medium; FA+ cells) or low levels of the receptor (produced by culturing the cells in normal growth medium; FA− cells) (2). For this, the two cell types were exposed to 1 μM of each type of the NPs for 2 h at 37°C and viewed under a confocal laser-scanning fluorescence microscope. Only the FA+ cells were shown to bind the NPAPF-PEG-FA NPs and to generate an intense fluorescence signal. Exposure of the FA+ cells to excess FA (concentration not mentioned) prior to the addition of NPAPF-PEG-FA NPs was reported to reduce the intensity of the fluorescence signal from the cells, indicating that the NPAPF-PEG-FA NPs specifically targeted the FA receptor in the FA+ cells. From this study, the investigators concluded that the NPAPF-PEG NPs can be modified to target cellular components for the detection and visualization of specific cell types (2) because the Fr is usually overexpressed in tumor cells and activated macrophages, but is expressed at low levels in healthy tissues (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20rodentia&cmd=DetailsSearch)]

The biodistribution of NPAPF-PEG NPs was investigated in Balb/c mice bearing A549 cell tumors (2). The animals (n = 3 mice/time point) were intravenously injected with 93 μM NPAPF-PEG NPs and euthanized at different time points ranging from 1 h postinjection (p.i.) to 48 h p.i., and fluorescence images of the organs of interest were acquired. The fluorescence intensity of each organ was calculated from the images to obtain a semi-quantitative biodistribution of the NPs, and the results were presented as percent of injected dose per gram tissue (% ID/g). At 1 h p.i., the accumulation of NPs in the liver, tumor, intestines, stomach, and kidney was 17.4% ID/g, 17.2% ID/g, 16% ID/g, 13% ID/g, and 8% ID/g, respectively. The accumulation of NPs in all other organs was reported to be <7% ID/g. At 12 h p.i., the uptake of NPs in the liver and the tumor was 25.2% ID/g and 29.5% ID/g NPs, respectively, and all other organs showed an accumulation varying from ~2% ID/g (heart) to ~10% ID/g (intestines). The blood circulation half-life of the NPAPF-PEG NPs was determined to be ~3 h. From this study, the investigators concluded that the uptake of NPAPF-PEG NPs in the cancerous lesions was due to the enhanced permeability and retention (EPR) effect in the tumor blood vessels (2). (For information regarding the EPR effect see Fang et al. (6).)

For whole-body imaging of the animals (number of animals not reported), the mice were injected with NPAPF-PEG NPs as before, and fluorescence images of the rodents were acquired at 12 h p.i (2). Only the tumors were reported to be visible in the animals at this time point.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=NPAPF%20nanoparticle%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Luo S., Zhang E., Su Y., Cheng T., Shi C. (2011). A review of NIR dyes in cancer targeting and imaging. Biomaterials.
2 Yang Y., An F., Liu Z., Zhang X., Zhou M., Li W., Hao X., Lee C.S. (2012). Ultrabright and ultrastable near-infrared dye nanoparticles for in vitro and in vivo bioimaging. Biomaterials.
3 Hong Y., Lam J.W., Tang B.Z. (2009). Aggregation-induced emission: phenomenon, mechanism and applications. Chem Commun (Camb).
4 Merian J., Gravier J., Navarro F., Texier I. (2012). Fluorescent nanoprobes dedicated to in vivo imaging: from preclinical validations to clinical translation. Molecules.
5 Muller C., Vlahov I.R., Santhapuram H.K., Leamon C.P., Schibli R. (2011). Tumor targeting using 67Ga-DOTA-Bz-folate--investigations of methods to improve the tissue distribution of radiofolates. Nucl Med Biol.
6 Fang J., Nakamura H., Maeda H. (2011). The EPR effect: Unique features of tumor blood vessels for drug delivery, factors involved, and limitations and augmentation of the effect. Adv Drug Deliv Rev.